# cypate-D: -(+)-glucosamine (cyp-GlcN), and D: -(+)-glucosamine-cypate-D: -(+)-glucosamine (cyp-2GlcN)

Chemical name: | cypate-D: -(+)-glucosamine (cyp-GlcN), and D: -(+)-gluosamine-cypate-D: -(+)-glucosamine (cyp-2GlcN)
Abbreviated name: | cyp-GlcN and cyp-2GlcN
Synonym:
Agent Category: | Compound
Target: | Glucose transporter protein 1 (GLUT1)
Target Category: | Transporter
Method of detection: | Near-infrared fluorescence (NIRF) imaging; optical imaging
Source of signal / contrast: | Cypate
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=glucose%20metabolism%20in%20tumors&cmd=DetailsSearch)]

Increased nutritional requirements are a characteristic feature of neoplastic tumor cells, and because these lesions do not rely on mitochondrial oxidation for energy, most of the energy in these cells is generated through glycolysis (1). To keep up with the high nutritional and energy needs of a malignant tumor, the transformed cells in the lesion show a 20- to 30-fold higher rate of glucose uptake and glycolysis compared with normal cells. As a consequence, to meet the increased demand for glucose, the facultative glucose transport proteins (GLUTs; there are 14 known isoforms of these proteins, designated GLUT1 through GLUT14) that facilitate glucose uptake are upregulated on the plasma membranes of the tumor cells (2). In general, GLUT1 and GLUT3 are able to transport glucosamine (GlcN) in addition to glucose and are overexpressed in the different cancer types, including prostate cancer. In addition, an elevated expression of these transporters correlates with the malignant potential of the lesions and indicates a poor prognosis for the patient (2). Among the different glucose transporters, GLUT2 and GLUT4 can also transport GlcN, and both of these isoforms are transcriptionally repressed by the p53 protein, a tumor suppressor protein that regulates the cell cycle and promotes apoptosis (3). GLUT1 and GLUT4 exhibit a similar affinity for glucose and GlcN, but GLUT2 has an approximate 20-fold higher affinity for GlcN than for glucose (3). The PC3 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1435&Template=cellBiology) human prostate cancer cell line does not express the p53 protein, and an increased expression of GLUT1 has been observed in these cells (3). Therefore, an imaging probe derived from GlcN would probably accumulate rapidly in tumors generated from the PC3 cells (3).

Currently, 2-deoxy-2-[^18^F]fluoro-D-glucose ([^18^F]-FDG), a glucose analog, is commonly used with positron emission tomography (PET) to detect, stage, and monitor cancers after therapy [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FDG%20and%20cancer&cmd=DetailsSearch)]. A major limitation of using [^18^F]-FDG to detect and monitor cancers is that this probe often generates false positive results (4). The main disadvantages of imaging with PET are that this technique involves the use of radionuclides that have a very short half-life and that the radiolabeled compounds used for this procedure have very high specific activities, which may expose the patient to an abnormal dose of radiation. As an alternative, there is much interest to develop probes that contain cyanine fluorophores, such as the cypate dye (cyp), because these fluorophores are visible in the near-infrared (NIR) wavelength of light and can be used for the noninvasive optical imaging of targeted tissues. The advantages of using cyp are that the compound has very low autofluorescence, absorption, and scattering within the excitation and emission ranges of the wavelength and that photons emitted from the dye can travel several centimeters through the tissue (3). Korotcov et al. investigated the in vitro and in vivo applications of cypate conjugated either to a single molecule of GlcN (cypate-D-(+)-GlcN; cyp-GlcN) or to two molecules of GlcN (D-(+)-glucosamine-cypate-D-(+)-glucosamine; cyp-2GlcN) to visualize luciferase-expressing PC3 cell (PC3-luc) xexograft tumors in mice (3). The biodistribution of cyp-GlcN and cyp-2GlcN was also studied in these animals.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Glucose%20transporters%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Glucose transporters in Online Mendelian Inheritance in Man (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Glucose%20transporters%20)) database

GLUT2 in Gene database (http://www.ncbi.nlm.nih.gov/gene/6514); Gene ID: 6514

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cyp-GlcN%20synthesis&cmd=DetailsSearch)]

The synthesis and purification of cyp-GlcN and cyp-2GlcN have been described by Ye et al. (5). The final yields of the compounds after the synthesis were >80%. The identity and purity (not reported) of the compounds were confirmed with electrospray mass spectrometry, nuclear magnetic resonance, and high-performance liquid chromatography. The number of cyp molecules per GlcN was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cyp-GlcN%20in%20vitro&cmd=DetailsSearch)]

The cellular uptake of cyp, cyp-GlcN, and cyp-2GlcN was investigated by exposing PC3-luc cells to the probes in the presence or absence (cell growth medium alone; controls) of 1 mM D-GlcN, 5 mM D-GlcN, 5 mM L-glucose (L-Glc), 25 mM L-Glc, 5 mM D-glucose (D-Glc), 25 mM D-Glc, or 25 mM N-acetyl-D-glucoseamine (GlcNAc) (3). Fluorescence microscopy showed that the dye alone and the dye conjugates were distributed in the entire cytoplasm, and no probe was visible in the nucleus or the periphery of the cells. The uptake of the fluorescent agents was reported to be cyp-2GlcN > cyp-GlcN > cyp, both in the presence or absence of the competing carbohydrates (P > 0.05). This indicated that the GLUT-mediated transport of cyp, cyp-GlcN, and cyp-2GlcN into the cells was either not completely inhibited by the presence of excess concentrations of the sugars or the dye-conjugated GlcNs were not transported into the cells through the GLUT system. The investigators suggested that more studies were necessary to delineate the mechanism of cyp, cyp-GlcN, and cyp-2GlcN uptake in the PC3 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cyp-GlcN%20rodentia&cmd=DetailsSearch)]

The ex vivo biodistribution of cyp, cyp-GlcN, and cyp-2GlcN was investigated in mice bearing PC3-luc cell tumors (3). The animals (number per group not reported) were injected with the probes (10 nmol) through the tail vein, and whole-body dynamic fluorescence images of the rodents were acquired at time points ranging from 10 min postinjection (p.i.) to 20–30 days p.i. as described elsewhere (3). Signal intensities from the images were reported as photons per second per centimeter square per steradian (p/s/cm^2^/sr). The tumor/muscle (T/M) ratios for cyp-2GlcN, cyp-GlcN, and cyp were 7.8, 3.8, and 2.0, respectively, at 24 h p.i., indicating that the uptake of cyp-2GlcN in the tumor cells was higher than that of either cyp-GlcN or cyp. With cyp-2GlcN, the T/M ratio was ~3.7 at 20 d p.i., indicating that this derivative of cyp had a long retention time in the tumors. However, the retention of cyp-2GlcN in the kidneys and the liver of the mice (~10^8^ p/s/cm^2^/sr in each organ) was higher than that of either cyp or cyp-GlcN (~7.1 p/s/cm^2^/sr in each organ/probe), even at 500 h p.i. This indicated that the dye and its carbohydrate conjugates were excreted through the urinary and biliary systems in the rodents.

To determine the in vivo tumor uptake specificity of cyp-2GlcN, mice bearing PC3-luc cell tumors (n = 6 animals/group) were given an intraperitoneal injection of either D-Glc (2 g/kg body weight (BW)), D-GlcN (0.5 g/kg BW), or GlcNAc (2 g/kg BW) 30 min before the administration of cyp-2GlcN through the tail vein (3). Fluorescence images of the rodents acquired at 24 h p.i. showed that pretreatment of the animals with D-Glc did not alter the uptake of cyp-2GlcN in the various organs, including tumors, of the animals as observed earlier in the in vitro study. The in vivo uptake of cyp-2GlcN was enhanced by the pretreatment with D-GlcN, suggesting that this carbohydrate activated the transport of GlcN and its derivatives into the different organs and tumors in the mice. Only GlcNAc inhibited the uptake of cyp-2GlcN in the various tissues and the tumors of the animals. This observation was in contrast to the results obtained during the in vitro study. The investigators suggested that the in vivo inhibition of cyp-2GlcN by GlcNAc was probably due to the higher concentration of GlcNAc (2 g/kg BW) used in this study compared with the concentration used for the in vitro experiments (10 nmol).

In another study, the mice (n = 3 animals/group) were injected with cyp, cyp-GlcN, or cyp-2GlcN as before, and the fluorescence intensities of the PC3 cell xenograft tumors were compared with those of the surrounding tissues for up to 10 h p.i. (cyp), 24 h p.i. (cyp-GlcN), and 45 h p.i. (cyp-2GlcN) (3). The maximum fluorescence intensities of the tumors with cyp, cyp-GlcN, or cyp-2GlcN were 4.7 × 10^7^ p/s/cm^2^/sr, 1.35 × 10^8^ p/s/cm^2^/sr, and 9.6 × 10^9^ p/s/cm^2^/sr at 1 min p.i., 30 min p.i., and 60 min p.i., respectively. In addition, the residence half-lives of cyp, cyp-GlcN, and cyp-2GlcN in the tumors were 15 min, 1.7 h, and 15 h, respectively. This indicated that addition of the GlcN moieties to cyp increased the retention time of the fluorescence probe in the lesions.

To determine the targeting specificity of cyp-2GlcN to the PC3-luc xenograft tumors, the mice (number of animals not reported) were administered 10 nmol of cyp-GlcN or cyp-2GlcN through the tail vein, and whole-body fluorescence images of the rodents were acquired for up to 30 days p.i (3). Between the two NIRF probes, cyp-2GlcN had a higher tumor specificity and retention time compared with the surrounding tissues. With cyp-2GlcN, the maximum fluorescence intensity of the tumor was observed at 24 h p.i., and the lesion was visible for up to 30 days p.i. Fluorescence was evident in the liver and kidneys of the mice for up to 24 h p.i., and the signal from these organs was observed to gradually decrease up to 96 h p.i.

From these studies, the investigators concluded that cyp-GlcN and cyp-2GlcN were suitable to detect prostate cancer cell derived tumors in mice (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cyp-GlcN%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cyp-GlcN%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cyp-GlcN%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported in part by grant RCMI 2G12RR003048 from the National Institutes of Health and the National Center for Research Resources.

## References

1 Jozwiak P., Krzeslak A., Pomorski L., Lipinska A. (2012). Expression of hypoxia-related glucose transporters GLUT1 and GLUT3 in benign, malignant and non-neoplastic thyroid lesions. Mol Med Report.
2 Krzeslak A., Wojcik-Krowiranda K., Forma E., Jozwiak P., Romanowicz H., Bienkiewicz A., Brys M. (2012). Expression of GLUT1 and GLUT3 glucose transporters in endometrial and breast cancers. Pathol Oncol Res.
3 Korotcov A.V., Ye Y., Chen Y., Zhang F., Huang S., Lin S., Sridhar R., Achilefu S., Wang P.C. (2012). Glucosamine-linked near-infrared fluorescent probes for imaging of solid tumor xenografts. Mol Imaging Biol.
4 Adejolu M., Huo L., Rohren E., Santiago L., Yang W.T. (2012). False-positive lesions mimicking breast cancer on FDG PET and PET/CT. AJR Am J Roentgenol.
5 Ye Y., Bloch S., Kao J., Achilefu S. (2005). Multivalent carbocyanine molecular probes: synthesis and applications. Bioconjug Chem.